# ^111^In-Diethylenetriaminepentaacetic acid-benzyl-succinamido-Lys-IRDye800-c(Arg-Gly-Asp-D-Phe-Lys)

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-benzyl-succinamido-Lys-IRDye800-c(Arg-Gly-Asp-D-Phe-Lys)
Abbreviated name: | ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK)
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | SPECT, gamma planar and optical, near-infrared (NIR) fluorescence
Source of signal: | ^111^In and IRDye800
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye800%20and%20RGD)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals (4, 5).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (6). Integrins consist of an α and a β subunit, and they are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (7-12). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents and its agonists are being studied as angiogenic agents for coronary angiogenesis (11, 13, 14). A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for tumor imaging and tumor angiogenesis (15).

Most of the cyclic RGD peptides are composed of five amino acids. Haubner et al. (16) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (50% inhibition concentration (IC_50_), 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (17). Li et al. (18) reported the development of ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK), a multimodality imaging agent for imaging α_v_β_3_ expression on breast tumors; single-photon emission computed tomography (SPECT) imaging used ^111^In-DTPA-Bz-SA and NIR imaging used IRDye800.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye800%20and%20RGD%20and%20synthesis)]

Li et al. (18) conjugated IRDye800-N-hydroxysuccinimide ester to the free ω-NH_2_ group of Lys in DTPA-Bz-SA-Lys-c(RGDfK) by incubation in basic solution (pH 8.5) for 2 h. Unlabeled DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) in 0.1 N sodium acetate was mixed with an aqueous solution of ^111^InCl_3_ for 15 min to form ^111^In- DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) with a specific activity of 2.22 MBq/nmol (0.06 mCi/nmol) and a radiochemical purity of >95. No free ^111^In^3+^ ions were found in the preparation. The molar ratio of IRDye800 to c(RGDfK) was ~1. DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) had a maximal excitation wavelength of 764 nm and a maximal emission wavelength of 794 nm; these values are similar to those for IRDye800. DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) (1 µM) had 70% of the signal intensity observed with IRDye800 (1 µM).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye800%20and%20RGD%20and%20in%20vitro)]

Li et al. (18) performed cell-adhesion assays to vitronectin using human melanoma cancer cell line M21 (α_v_β_3_-positive). Binding of M21 cells to vitronectin was blocked by DTPA-Bz-SA-Lys-IRDye800-c(RGDfK), DTPA-Bz-SA-Lys-IRDye800-c(RGDfK), and c(RGDfK) in a dose-dependent manner with IC_50_ values of 3.86 ± 0.36 μM, 3.78 ± 0.28 μM, and 3.16 ± 0.09 µM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye800%20and%20RGD%20and%20rodentia)]

Li et al. (18) studied the accumulation of ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) in nude mice bearing M21 (α_v_β_3_-positive) and M21-L (α_v_β_3_-negative) tumors. ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) (0.4 nmol/mouse) was injected intravenously into tumor-bearing nude mice (n = 3/group). ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) tumor uptake (% injected dose per gram (% ID/g)) at 2, 4, 24, and 48 h after injection was significantly higher in M21 tumors (1.47 ± 0.12, 1.68 ± 0.14, 1.41 ± 0.49, and 0.84 ± 0.06, respectively) than in M21-L tumors (0.5 ± 0.07, 0.6 ± 0.08, 0.49 ± 0.04 and 0.23 ± 0.02, respectively). The kidney was the organ with the highest uptake. Moderate uptake was observed in the liver and spleen. The radioactivity in the blood and other organs and tissues continued to decrease from 2 min after injection. The M21 tumor/blood, M21 tumor/muscle, and M21 tumor/M21-L tumor ratios at 24 h after injection were 47.0, 5.0, and 2.9, respectively. ^111^In-DTPA-Bz-SA-Lys-c(RGDfK) showed a biodistribution pattern similar to ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK). Gamma and optical imaging at 24 h after injection showed complementary and distinct signals in the tumors and kidneys. The M21/M21-L ratio was 1.7 for optical imaging and 1.5 for gamma imaging. Pretreatment with c(RGDfK) (600 nmol/mouse, 60 min before ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) injection) inhibited the ^111^In-DTPA-Bz-SA-Lys-IRDye800-c(RGDfK) binding in the M21 tumor by ~90% but caused little inhibition in the M21-L tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye800%20RGD%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye800%20RGD%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye800%20RGD%20and%20human)]

No publication is currently available.

## NIH Support

R01 EB00174, U54 CA90810

1. Achilefu, S., Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat, 2004. 3(4): p. 393-409.

2. Ntziachristos, V., C. Bremer, and R. Weissleder, Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol, 2003. 13(1): p. 195-208.

3. Becker, A., C. Hessenius, K. Licha, B. Ebert, U. Sukowski, W. Semmler, B. Wiedenmann, and C. Grotzinger, Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol, 2001. 19(4): p. 327-31.

4. Robeson, W., V. Dhawan, A. Belakhlef, Y. Ma, V. Pillai, T. Chaly, C. Margouleff, D. Bjelke, and D. Eidelberg, Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med, 2003. 44(6): p. 961-6.

5. Tung, C.H., Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers, 2004. 76(5): p. 391-403.

6. Hynes, R.O., Integrins: versatility, modulation, and signaling in cell adhesion. Cell, 1992. 69(1): p. 11-25.

7. Jin, H. and J. Varner, Integrins: roles in cancer development and as treatment targets. Br J Cancer, 2004. 90(3): p. 561-5.

8. Varner, J.A. and D.A. Cheresh, Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol, 1996: p. 69-87.

9. Wilder, R.L., Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis, 2002. 61 Suppl 2: p. ii96-9.

10. Grzesik, W.J., Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz), 1997. 45(4): p. 271-5.

11. Kumar, C.C., Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets, 2003. 4(2): p. 123-31.

12. Ruegg, C., O. Dormond, and A. Foletti, Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target? Endothelium, 2002. 9(3): p. 151-60.

13. Kerr, J.S., S.A. Mousa, and A.M. Slee, Alpha(v)beta (3) integrin in angiogenesis and restenosis. Drug News Perspect, 2001. 14(3): p. 143-50.

14. Mousa, S.A., alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev, 2003. 23(2): p. 190-9.

15. Haubner, R. and H.J. Wester, Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des, 2004. 10(13): p. 1439-55.

16. Haubner, R., H.J. Wester, F. Burkhart, R. Senekowitsch-Schmidtke, W. Weber, S.L. Goodman, H. Kessler, and M. Schwaiger, Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med, 2001. 42(2): p. 326-36.

17. Chen, X., R. Park, A.H. Shahinian, M. Tohme, V. Khankaldyyan, M.H. Bozorgzadeh, J.R. Bading, R. Moats, W.E. Laug, and P.S. Conti, 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol, 2004. 31(2): p. 179-89.

18. Li, C., W. Wang, Q. Wu, S. Ke, J. Houston, E. Sevick-Muraca, L. Dong, D. Chow, C. Charnsangavej, and J.G. Gelovani, Dual optical and nuclear imaging in human melanoma xenografts using a single targeted imaging probe. Nucl Med Biol, 2006. 33(3): p. 349-58.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
7 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
8 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
9 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
10 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
11 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
12 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
13 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
14 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
15 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
16 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
17 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
18 Li C., Wang W., Wu Q., Ke S., Houston J., Sevick-Muraca E., Dong L., Chow D., Charnsangavej C., Gelovani J.G. (2006). Dual optical and nuclear imaging in human melanoma xenografts using a single targeted imaging probe. Nucl Med Biol.